# Cy5.5-8-Amino-octanoic acid-Ser-Cys-Pro-Pro-Trp-Gln-Glu-Trp-His-Asn-Phe-Met-Pro-Phe-NH_2_

Chemical name: | Cy5.5-8-Amino-octanoic acid-Ser-Cys-Pro-Pro-Trp-Gln-Glu-Trp-His-Asn-Phe-Met-Pro-Phe-NH_2_
Abbreviated name: | Cy5.5-Aoc-EGBP
Synonym: | EGBP-Aoc-Cy5.5
Agent category: | Peptide
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGBP)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging human breast cancer (12-16). C225, an anti-EGFR (HER1), mouse-human chimeric, monoclonal IgG_1_ antibody, also known as erbitux and cetuximab, was radiolabeled for imaging EGFR expression on solid tumors. However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for EGFR and HER2, based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A, was constructed (17). Affibody molecules exhibit high binding affinity to EGFR and HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image EGFR and HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20EGFR)]. Jeong et al. (18) identified one 12-mer peptide, Pro-Pro-Trp-Gln-Glu-Trp-His-Asn-Phe-Met-Pro-Phe-NH_2_ (EGBP), with specific binding activity for human EGFR using phage display screening. The linker 8-mino-octanoic acid-Ser-Cys, (Aoc-SC) was added to the C-terminus of EGBP for Cy5.5 labeling. Cy5.5-8-Amino-octanoic acid-Ser-Cys-Pro-Pro-Trp-Gln-Glu-Trp-His-Asn-Phe-Met-Pro-Phe-NH_2_ (Cy5.5-Aoc-EGBP) was evaluated for use with in vivo near-infrared (NIR) fluorescence imaging in mice with EGFR-positive tumors.

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22421431)]

8-Aoc-SC-EGBP (1,946 Da) was prepared with an automated solid-phase peptide synthesizer (18), with 75%–85% yield and >95% purity after purification with high-performance liquid chromatography (HPLC). Cy5.5-Mono-maleimide and 8-Aoc-SC-EGBP (~1:1 molar ratio) were incubated in dimethyl sulfoxide and triethylamine for 20 h at 25°C. Cy5.5-Aoc-EGBP (2,985 Da) was isolated with >95% purity after HPLC purification. Mass spectroscopy analysis confirmed 1:1 Cy5.5 conjugation. Spectrum analysis showed that Cy5.5-Aoc-EGBP exhibited maximal fluorescence absorption (680 nm) and emission (696 nm) characteristics similar to those of free Cy5.5 dye.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22421431)]

Fluorescence microscopy analysis was performed in U87MG human glioblastoma cells (high EGFR expression) after incubation with 4 nmol Cy5.5-Aoc-EGBP for 60 min at 37°C (18). U87MG cells exhibited intensive fluorescence signal from the cell surface and cytoplasm. Co-incubation with 49 nmol non-labeled EGBP clearly decreased the signal.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22421431)]

Jeong et al. (18) performed NIR fluorescence imaging of nude mice (n = 3/group) bearing U87MG tumors at 0.5, 1, 2, 3, 4, 6, 8, 20, and 24 h after intravenous injection of 4 nmol Cy5.5-Aoc-EGBP. The accumulation of Cy5.5-Aoc-EGBP in U87MG tumors could be clearly visualized from 0.5 h to 24 h, with maximum contrast at 3 h. The tumor/background ratio was 85 at 3 h. The kidney accumulation of Cy5.5-Aoc-EGBP was slightly less than that of the tumor at the time points measured. No blocking studies or ex vivo NIR fluorescence imaging of tissues were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Jeong M.H., Kim K., Kim E.M., Cheong S.J., Lee C.M., Jeong H.J., Kim D.W., Lim S.T., Sohn M.H., Chung J. (2012). In vivo and in vitro evaluation of Cy5.5 conjugated epidermal growth factor receptor binding peptide. Nucl Med Biol.